# [^18^F]3-Fluoro-5-[(pyridin-3-yl)ethynyl]benzonitrile

Chemical name: | [^18^F]3-Fluoro-5-[(pyridin-3-yl)ethynyl]benzonitrile
Abbreviated name: | [^18^F]F-PEB
Synonym:
Agent Category: | Compound
Target: | Metabotropic glutamate subtype 5 (mGlu5) receptor
Target Category: | Receptor binding
Method of detection: | Positron Emission Tomography (PET)
Source of signal/contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=metabotropic%20glutamate%20receptor%20subtype%205%20%28mGluR5%29%20PET%20radiotracers)]

[^18^F]3-Fluoro-5-[(pyridin-3-yl)ethynyl]benzonitrile ([^18^F]F-PEB) is a radioligand developed for positron emission tomography (PET) imaging of metabotropic glutamate receptor subtype 5 (mGlu5) in the central nervous system (CNS) (1).

Glutamate is a major excitatory neurotransmitter at CNS synapses. Many neuroanatomical CNS projection pathways contain glutamatergic neurons (2). Glutamate produces its excitatory effects by acting on cell-surface ionotropic glutamate or metabotropic glutamate (mGlu) receptors (3). The mGlu receptors are G-protein-coupled receptors, and the eight mGlu receptor subtypes are further subdivided into groups I, II, and III. The group I receptors include mGlu1 and mGlu5, and they are found mostly in postsynaptic locations. The mGlu5 receptors are found with high to moderate density in the frontal cortex, caudate, putamen, nucleus accumbens, olfactory tubercle, hippocampus, and dorsal horn of the spinal cord, whereas the density in the cerebellum is low. These receptors are coupled to phospholipase C and up- or down-regulate neuronal excitability. They have been implicated in a variety of diseases in the CNS, including anxiety, depression, schizophrenia, Parkinson’s disease, and drug addiction or withdrawal. These receptors are also involved in the modulation of various pain states. They thus are attractive targets for therapeutic drug development.

PET and single-photon emission tomography of radioligands targeting mGlu5 receptors can visualize and study the CNS mGlu5 receptors in normal and pathologic states. Some mGlu5 antagonists have been successfully labeled, but their in vivo visualization has been hampered by high lipophilicity, unfavorable brain uptake kinetics, or a high metabolism (4, 5). 2-Methyl-6-(phenylethynyl)-pyridine (MPEP) and its methyl analog M-MPEP have been identified as potent and highly selective noncompetitive antagonists for mGlu5. Using the structure of MPEP as a base, Hamill et al. (1) and Patel et al. (5) designed several MPEP analogs as PET radiotracers; [^18^F]F-PEB was one of the compounds that showed high affinity for mGlu5 receptors with moderate lipophilicity.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=metabotropic%20glutamate%20receptor%20subtype%205%20%28mGluR5%29%20PET%20radiotracers%20AND%20synthesis)]

Hamill et al. (1) reported the radiosynthesis of [^18^F]F-PEB from the aryl chloride via a nucleophilic aromatic substitution reaction. The precursor, 3-chloro-5-[(pyridin-2-yl)ethynyl]benzonitrile, was obtained commercially. In the preparation, Kryptofix222 was added to the aqueous [^18^F]F− solution in a microwave cavity. The fluoride was dried under argon gas flow by use of microwave pulses (~45 W). The precursor, in dimethyl sulfoxide, was added to the microwave vial. The reaction mixture was then pulsed with the microwave 5 times at 5 s/pulse, with a 30-s pause between pulses. After cooling for 1 min, the reaction was diluted with water and then purified by high-performance liquid chromatography (HPLC). This procedure gave 518 MBq(14 mC) of [^18^F]F-PEB with a specific activity of 75.3 ± 9.7 TBq (2,034 ± 359 Ci)/mmol and a radiochemical purity >98%. The time of synthesis was ~ 45 min with a radiochemical yield of 4 ± 0.6% (n = 4) at the end of synthesis (uncorrected).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%5Bmetabotropic%20glutamate%20receptor%20subtype%205%20%28mGluR5%29%20PET%20radiotracers%20%5D%20AND%20in%20vitro)]

Patel et al. (5) used in vitro rat brain preparations to determine the in vitro mGlu5 binding parameters of unlabeled F-PEB. [^3^H]MethoxyPyEP, a mGlu5 antagonist, was used in the equilibrium competition studies. The B_max_ for the rat frontal cortex was reported to be 64.7 fmol/mg of tissue (6). The K_i_ of F-PEB determined from rat cortical membranes was 0.20 ± 0.01 nM (n = 3), and the partition coefficient (log P) was 2.8 (octanol/buffer, pH 7.4). Hamill et al. (1) reported that the 50% inhibitory concentration (IC_50_; human mGlu5 Ca^2+^ flux assay) was 0.66 ± 0.2 nM (n = 2).

Using a rapid in vitro binding assay they had developed, Patel et al. (7) determined the in vitro regional distribution of [^18^F]F-PEB in rat and rhesus monkey brain sections. Rat and rhesus brain sections were incubated with [^18^F]F-PEB and assayed for 20 min, using a no-wash protocol. The percentages of specific binding (n ≥ 2) at 20 min were 77 ± 8.1 and 69 ± 22 for rat and rhesus caudate sections, respectively.

In vitro autoradiographic studies (1) of [^18^F]F-PEB were carried out in rhesus monkey brain slices (from a single monkey). Good specific to nonspecific regioselective labeling with reasonable binding was found in cortex, caudate, putamen, amygdale, hippocampus, and most thalamic nuclei. The cerebellar layers showed less density of binding. In a saturation binding experiment, the B_max_ values for mGlu5 were determined to be 63 and 24 nM in the rhesus caudate and cerebellum, respectively. In vitro metabolism of F-PEB was studied by incubation of the radiotracer with human and monkey liver microsomes. Liquid chromatography-tandem mass spectrometry showed that the radiotracer was metabolized slowly by human microsomes. Approximately 70% of the intact compound remained at the end of 30 min. In contrast, the compound was metabolized much faster by monkey liver microsomes: only ~30% of the intact compound remained at the end of 30 min.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%5Bmetabotropic%20glutamate%20receptor%20subtype%205%20%28mGluR5%29%20PET%20radiotracers%20%5D%20AND%20%28%22rodentia%22%5BMeSH%20Terms%5D%20OR%20rodentia%5BText%20Word%5D%25)]

Patel et al. (5) assessed the in vivo distribution of [^18^F]F-PEB via micro-PET imaging in the rat brain. The rat received 18.5 MBq (0.5 mCi) of [^18^F]F-PEB (specific activity = 74 TBq (2,000 Ci)/mmol) by intravenous injection. [^18^F]F-PEB exhibited an excellent in vivo specific signal-to-noise ratio. The specific binding and signal-to-noise ratio were reasonably well maintained over 90 min. The corpus striatum/cerebellum ratio was 7.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%5Bmetabotropic%20glutamate%20receptor%20subtype%205%20%28mGluR5%29%20PET%20radiotracers%20%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%5Bmetabotropic%20glutamate%20receptor%20subtype%205%20%28mGluR5%29%20PET%20radiotracers%20%5D%20AND%20%28primate%20NOT%20human%29)]

PET imaging with [^18^F]F-PEB was carried out in three rhesus monkeys (1). Each monkey received ~185 MBq (5 mCi) of the radiotracer. PET showed rapid brain uptake of [^18^F]F-PEB radioactivity and substantial mGlu5-specific signals in all gray matter regions, including the cerebellum. The wash-out from the brain was relatively slow and thus produced large, long-lived specific signals. The nonspecific signal was determined from the radioactivity in the white matter with a blocking dose of 3 mg/kg 3-[(2-methyl-1,3-thiazol-4-yl)ethynyl]pyridine (MTEP), a selective, high-affinity mGlu5 ligand. The total/nonspecific signal ratio at 85 min was 8.1. Coregistered magnetic resonance imaging/PET imaging confirmed that the radioactivity uptake was in the striatum, cortical regions, and cerebellum. The highest concentration of radioactivity was observed in the striatum with ~4.2 standard uptake value (SUV) units at ~55 min. Radioactivity uptake was lower in the frontal cortex and even lower in the cerebellum. These uptakes were blocked by MTEP pretreatment. The distribution of radioactivity seen in PET imaging was consistent with the in vitro autoradiography pattern.

Hamill et al. (1) also used HPLC analyses of plasma samples obtained from the monkeys during the above imaging studies to study in vivo [^18^F]F-PEB metabolism. Only one polar metabolite, which could not cross the blood-brain barrier, was observed. The percentages of [^18^F]F-PEB that remained unchanged were 95.5 ± 1.3, 85.4 ± 3.0, 77.7 ± 3.5, and 62.4 ± 4.5 at 5, 15, 30, and 90 min after administration, respectively.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%5Bmetabotropic%20glutamate%20receptor%20subtype%205%20%28mGluR5%29%20PET%20radiotracers%20%5D%20AND%20human)]

No publication is currently available.

## References

1 Hamill T.G., Krause S., Ryan C., Bonnefous C., Govek S., Seiders T.J., Cosford N.D., Roppe J., Kamenecka T., Patel S., Gibson R.E., Sanabria S., Riffel K., Eng W., King C., Yang X., Green M.D., O'Malley S.S., Hargreaves R., Burns H.D. (2005). Synthesis, characterization, and first successful monkey imaging studies of metabotropic glutamate receptor subtype 5 (mGluR5) PET radiotracers. Synapse.
2 Pin J.P., Duvoisin R. (1995). The metabotropic glutamate receptors: structure and functions. Neuropharmacology.
3 Slassi A., Isaac M., Edwards L., Minidis A., Wensbo D., Mattsson J., Nilsson K., Raboisson P., McLeod D., Stormann T.M., Hammerland L.G., Johnson E. (2005). Recent advances in non-competitive mGlu5 receptor antagonists and their potential therapeutic applications. Curr Top Med Chem.
4 Ametamey S.M., Kessler L.J., Honer M., Wyss M.T., Buck A., Hintermann S., Auberson Y.P., Gasparini F., Schubiger P.A. (2006). Radiosynthesis and Preclinical Evaluation of 11C-ABP688 as a Probe for Imaging the Metabotropic Glutamate Receptor Subtype 5. J Nucl Med.
5 Patel S., Ndubizu O., Hamill T., Chaudhary A., Burns H.D., Hargreaves R., Gibson R.E. (2005). Screening cascade and development of potential Positron Emission Tomography radiotracers for mGluR5: in vitro and in vivo characterization. Mol Imaging Biol.
6 Patel S., Krause S.M., Hamill T., Chaudhary A., Burns D.H., Gibson R.A. (2003). In vitro characterization of [3H]MethoxyPyEP, an mGluR5 selective radioligand. Life Sci.
7 Patel S., Hamill T., Hostetler E., Burns H.D., Gibson R.E. (2003). An in vitro assay for predicting successful imaging radiotracers. Mol Imaging Biol.